# ^99m^Tc-Fucoidan, a polysaccharidic ligand of P-selectin

Chemical name: | ^99m^Tc-Fucoidan, a polysaccharidic ligand of P-selectin
Abbreviated name: | ^99m^Tc-Fucoidan
Synonym:
Agent category: | Polysaccharide
Target: | P-selectin
Target category: | Receptor
Method of detection: | single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=200553), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=6031196) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=6403) for more information about P-selectin.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20and%20P-selectin)]

Endothelial cells are important cells in inflammatory responses (1, 2). Bacterial lipopolysaccharide, virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and secretion of other cytokines and chemokines. Leukocyte emigration from blood is dependent on rolling of leukocytes along endothelial cell surfaces and subsequent adherence to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic to leukocytes attracting them to sites of inflammation and tissue injury. The movement of leukocytes and tumor cells through endothelial junctions into the extravascular space is highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3, 4).

P-selectin is found on the cell surface of endothelial cells and platelets (5, 6). It binds to glycoprotein on the cell surface of leukocytes. IL-1 and TNFα, released from inflammatory and ischemic stimuli, stimulate expression of P-selectin and other adhesion molecules on the vascular endothelial cells leading to leukocyte adhesion to the activated endothelium and platelets. P-selectin and other adhesion molecules are involved in rolling and arresting leukocytes on the endothelium prior to leukocyte migration into the extravascular space. Fucoidan (a sialy-Lewis^x^ mimetic) is a sulfated polysaccharide in brown seaweed (7, 8). Fucoidan binds to P-selectin with high affinity and exerts antagonism of selective function on myocardial ischemia-perfusion injury models in rats (9) and pigs (10). Rouzet et al. (11) evaluated ^99m^Tc-fucoidan as a noninvasive agent for P-selectin expression in vascular endothelial cells of inflamed and damaged tissues and in platelet-rich arterial thrombus.

### Related Resource Links:

- Chapters in MICAD (P-selectin (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=P-selectin%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (P-selectin (http://www.ncbi.nlm.nih.gov/gene/6403))
- Articles in Online Mendelian Inheritance in Man (OMIM) (P-selectin (http://omim.org/entry/173610))
- Clinical trials (Fucoidan (http://www.clinicaltrials.gov/ct2/results?term=fucoidan))
- Drug information in FDA (Fucoidan (http://google2.fda.gov/search?q=fucoidan&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT)]

Rouzet et al. (11) prepared ^99m^Tc-fucoidan by mixing 1.5 nmol fucoidan (7.2 kDa) with 740 MBq (20 mCi) ^99m^Tc-pertechnetate, stannous chloride, and potassium borohydride for 1 h at room temperature. The radiochemical purity was >99%. The yield, specific activity and stability of ^99m^Tc-fucoidan were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT%20and%20in%20vitro)]

Rouzet et al. (11) showed that there was a 10-fold increase in ^99m^Tc-fucoidan binding to a fibrinogen-coated plate with adhered platelets compared versus binding to a fibrinogen-coated plate without adhered platelets. No blocking studies were performed with unlabeled fucoidan.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT%20and%20rodentia)]

Rouzet et al. (11) performed ex vivo biodistribution of 50 MBq (1.35 mCi) ^99m^Tc-fucoidan in normal male rats (n = 4/group). Radioactivity was cleared from the blood with an initial half-life of 19 min and a second half-life of 351 min. The organ with the highest accumulation at 2 h after injection was the kidney (4.8% injected dose/gram (ID/g), followed by the liver (0.62% ID/g), blood (0.62% ID/g), bone (0.56% ID/g), thyroid (0.25% ID/g), spleen (0.21% ID/g), lung (0.17% ID/g), heart (0.11% ID/g), muscle (0.04% ID/g), and brain (0.01% ID/g).

Rouzet et al. (11) performed scintigraphy imaging studies of ^99m^Tc-fucoidan in rats with myocardial ischemia-reperfusion (n = 7) after coronary artery occlusion. Static images were obtained at 120 min after ^99m^Tc-fucoidan injection. The ischemia/non-ischemia ratio was 4.1 (2.3–6.2). Autoradiography studies of the excised tissues showed the ischemia/non-ischemia ratio to be 24.9 (4.1–44.0). There was a good correlation between the ^99m^Tc-fucoidan accumulation and the area of injured myocardium measured with autoradiography (P < 0.05). Immunohistochemistry analysis showed a co-localization of P-selectin with radioactivity in the vasculature in the ischemia area. Non-specific accumulation was assessed with injection of ^99m^Tc-aprotinin (a glycoprotein with a molecular weight of 6.5 kDa) as a control in two rats. No focal accumulation of radioactivity was detected with single-photon computed tomography or autography studies. In another study, accumulation of ^99m^Tc-fucoidan (120 min after injection) in platelet-rich arterial thrombi was measured in rats with abdominal aortic aneurysms (n = 9) and infective endocarditis (n = 6). The aneurysmal thrombi/control and vegetations (thrombi)/background ratios were 3.6 (2.2–8.5) and 5.2 (2.7–9.1), respectively. Autoradiography studies of the excised tissues showed the ratios to be 9.1 (6.3–15.8) and 17 (14–32), respectively. Immunohistochemistry analysis showed a co-localization of P-selectin with radioactivity in the affected regions. No direct blocking studies were performed with unlabeled fucoidan.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Fucoidan%20SPECT%20and%20human)]

No publication is currently available.

## References

1 Cybulsky, M.I., D. Won, and M. Haidari, Leukocyte recruitment to atherosclerotic lesions. Can J Cardiol, 200420 Suppl B: p. 24B-28B.
2 Wang H.B., Wang J.T., Zhang L., Geng Z.H., Xu W.L., Xu T., Huo Y., Zhu X., Plow E.F., Chen M., Geng J.G. (2007). P-selectin primes leukocyte integrin activation during inflammation. Nat Immunol.
3 Woollard K.J., Chin-Dusting J. (2010). P-selectin antagonism in inflammatory disease. Curr Pharm Des.
4 Laubli H., Borsig L. (2010). Selectins promote tumor metastasis. Semin Cancer Biol.
5 Chen M., Geng J.G. (2006). P-selectin mediates adhesion of leukocytes, platelets, and cancer cells in inflammation, thrombosis, and cancer growth and metastasis. Arch Immunol Ther Exp (Warsz).
6 Lowe J.B. (2003). Glycan-dependent leukocyte adhesion and recruitment in inflammation. Curr Opin Cell Biol.
7 Li B., Lu F., Wei X., Zhao R. (2008). Fucoidan: structure and bioactivity. Molecules.
8 Bachelet L., Bertholon I., Lavigne D., Vassy R., Jandrot-Perrus M., Chaubet F., Letourneur D. (2009). Affinity of low molecular weight fucoidan for P-selectin triggers its binding to activated human platelets. Biochim Biophys Acta.
9 Omata M., Matsui N., Inomata N., Ohno T. (1997). Protective effects of polysaccharide fucoidin on myocardial ischemia-reperfusion injury in rats. J Cardiovasc Pharmacol.
10 Barrabes J.A., Garcia-Dorado D., Mirabet M., Inserte J., Agullo L., Soriano B., Massaguer A., Padilla F., Lidon R.M., Soler-Soler J. (2005). Antagonism of selectin function attenuates microvascular platelet deposition and platelet-mediated myocardial injury after transient ischemia. J Am Coll Cardiol.
11 Rouzet F., Bachelet-Violette L., Alsac J.M., Suzuki M., Meulemans A., Louedec L., Petiet A., Jandrot-Perrus M., Chaubet F., Michel J.B., Le Guludec D., Letourneur D. (2011). Radiolabeled fucoidan as a p-selectin targeting agent for in vivo imaging of platelet-rich thrombus and endothelial activation. J Nucl Med.